# Cy5.5-Anti-ephrin receptor B4 (EphB4) humanized monoclonal antibody hAb47

Chemical name: | Cy5.5-Anti-ephrin receptor B4 (EphB4) humanized monoclonal antibody hAb47
Abbreviated name: | Cy5.5-hAb47
Synonym:
Agent category: | Peptide
Target: | Ephrin receptor B4 (EphB4)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure is not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47)]

The ephrin (Eph) receptors constitute the largest group in the receptor tyrosine kinase family (1, 2). The Eph receptors and their ligands (ephrins) mediate numerous biological processes in normal development, particularly in the nervous and cardiovascular systems (3-5). On the basis of their structures and sequence relationships, ephrins are divided into two classes: the ephrin-A class, Ephs that are anchored to the cell membrane by a glycosylphosphatidylinositol linkage, and the ephrin-B class, Ephs that are transmembrane proteins. The Eph family of receptors is divided into two groups, EphA and EphB, on the basis of the similarity of their extracellular domain sequences and their affinities for binding ephrin-A and ephrin-B ligands. The Eph receptors transmit forward signals via their kinase domains and reverse signals via their transmembrane ephrin ligands (6). EphB–ephrin-B interactions are capable of mediating bidirectional signaling events upon cell–cell contact, either into the receptor-expressing cell as "forward signaling" or into the ligand-expressing cell as "reverse signaling" (7).

Eph-2 is expressed on arterial and activated endothelial cells, whereas EphB4 is normally expressed on venous endothelial cells and various blood cells (8). EphB4 selectively binds to ephrin-2 to promote cell signaling and angiogenesis. EphB4 has been implicated in cancer progression and in pathological forms of angiogenesis. Overexpression of EphB4 has been observed in cancer cells and is associated with tumorigenesis via forward signaling and with angiogenesis via reverse signaling through Eph-2 interaction (9). EphB4 forward signaling stimulates cellular proliferation. Koolpe et al. (10) identified a 15-mer peptide, Tyr-Asn-Tyr-Leu-Phe-Ser-Pro-Asn-Gly-Pro-Ile-Ala-Arg-Ala-Trp (TNYL-RAW), to be a selective antagonist of EphB4 with the use of phage display screening. Xiong et al. (11) reported the development of ^64^Cu-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-TNYL-RAW (^64^Cu-DOTA-TNYL-RAW) for use with positron emission tomography (PET) imaging of EphB4 in nude mice bearing tumor xenografts. A monoclonal antibody mAb47 was found to have high affinity (0.8 nM) for the fibronectin-like extracellular domain of both human and mouse EphB4. Li et al. (12) conjugated Cy5.5 to the humanized Ab47 (hAb47) antibody to produce Cy5.5-hAb47 for use with near-infrared (NIR) fluorescence imaging of EphB4 expression in tumors.

### Related Resource Links:

- Chapters in MICAD (EphB4 (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=EphB4+AND+micad%5Bbook%5D))
- Gene information in NCBI (EphB4 (http://www.ncbi.nlm.nih.gov/gene?term=2050), Eph-B2 (http://www.ncbi.nlm.nih.gov/gene/1948))
- Articles in Online Mendelian Inheritance in Man (OMIM) (EphB4 (http://www.ncbi.nlm.nih.gov/omim/600011), Eph-B2 (http://www.ncbi.nlm.nih.gov/omim/600527))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47+synthesis)]

A solution of hAb47 (3.3. nmol) and Cy5.5-NHS (3.3 nmol) in borate buffer (pH 8.5) was incubated for 1.5 h at room temperature (12). Cy5.5-hAb47 was isolated with PD-10 column chromatography. Cy5.5-hIgG was prepared similarly as a control. Gel electrophoresis showed that both the heavy and the light chains of the antibodies were labeled with Cy5.5. The Cy5.5 moiety per antibody was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47%20in+vitro)]

Li et al. (12) performed binding experiments with Cy5.5-hAb47 immobilized with EphB4-HSA. Fluorescence signal increased with increasing amounts of Cy5.5-hAb47 (0.066–3.3 nmol). The immunoreactivity values for Cy5.5-hAB47 and Cy5.5-hIgG were 81.62 ± 2.08% and 0.024 ± 0.07%, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47+rodentia)]

Li et al. (12) performed in vivo optical imaging studies of Cy5.5-hAb47 or Cy5.5-hIgG (0.2 nmol/mouse) in nude mice (n = 6) bearing HT29 human colorectal tumors. Whole-body optical imaging scans were performed at 6, 24, 48, 72, 96, and 120 h after injection. Cy5.5-hAb47 exhibited a relatively low tumor fluorescence signal of ~1 × 10^9^ photons/s/cm^2^/sr at 6 h, and the signal increased to a plateau of ~2 × 10^9^ photons/s/cm^2^/sr at 48 h. Tumor accumulation of the control Cy5.5-IgG was low at 6 h (~0.6 × 10^9^ photons/s/cm^2^/sr) and reached a peak at 48 h (~0.8 × 10^9^ photons/s/cm^2^/sr). The accumulation of Cy5.5-hAb47 was significantly higher than that of Cy5.5-hIgG at all the time points studied (P < 0.05). Ex vivo imaging studies showed that the tumor fluorescence intensity of mice injected with Cy5.5-hAb47 was 0.8-fold higher than that of Cy5.5-hIgG at 120 h after injection. Of the major normal tissues, only the liver showed a moderate and similar accumulation of both tracers (~0.4 × 10^9^ photons/s/cm^2^/sr). No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=hAb47+human)]

No publication is currently available.

## NIH Support

R21 EB012294-01a1

## References

1 Dodelet V.C., Pasquale E.B. (2000). Eph receptors and ephrin ligands: embryogenesis to tumorigenesis. Oncogene.
2 Pasquale E.B. (1997). The Eph family of receptors. Curr Opin Cell Biol.
3 Adams R.H., Klein R. (2000). Eph receptors and ephrin ligands. essential mediators of vascular development. Trends Cardiovasc Med.
4 Cheng N., Brantley D.M., Chen J. (2002). The ephrins and Eph receptors in angiogenesis. Cytokine Growth Factor Rev.
5 Murai K.K., Pasquale E.B. (2011). Eph receptors and ephrins in neuron-astrocyte communication at synapses. Glia.
6 Noren N.K., Lu M., Freeman A.L., Koolpe M., Pasquale E.B. (2004). Interplay between EphB4 on tumor cells and vascular ephrin-B2 regulates tumor growth. Proc Natl Acad Sci U S A.
7 Pasquale E.B. (2010). Eph receptors and ephrins in cancer: bidirectional signalling and beyond. Nat Rev Cancer.
8 Pfaff D., Heroult M., Riedel M., Reiss Y., Kirmse R., Ludwig T., Korff T., Hecker M., Augustin H.G. (2008). Involvement of endothelial ephrin-B2 in adhesion and transmigration of EphB-receptor-expressing monocytes. J Cell Sci.
9 Noren N.K., Pasquale E.B. (2007). Paradoxes of the EphB4 receptor in cancer. Cancer Res.
10 Koolpe M., Burgess R., Dail M., Pasquale E.B. (2005). EphB receptor-binding peptides identified by phage display enable design of an antagonist with ephrin-like affinity. J Biol Chem.
11 Xiong C., Huang M., Zhang R., Song S., Lu W., Flores L., Gelovani J., Li C. (2011). In vivo small-animal PET/CT of EphB4 receptors using 64Cu-labeled peptide. J Nucl Med.
12 Li D., Liu S., Liu R., Park R., Hughes L., Krasnoperov V., Gill P.S., Li Z., Shan H., Conti P.S. (2013). Targeting the EphB4 Receptor for Cancer Diagnosis and Therapy Monitoring. Mol Pharm.